# Hyperpolarized sodium 1-[^13^C]pyruvate

Chemical name: | Hyperpolarized sodium 1-[^13^C]pyruvate
Abbreviated name: | HP[^13^C]Pyr
Synonym: | Sodium pyruvate-1-^13^C, Pyruvic acid-1-^13^C sodium
Agent category: | Small molecule
Target: | Other
Target category: | Other -metabolism
Method of detection: | Magnetic resonance spectroscopic imaging (MRSI), magnetic resonance imaging (MRI)
Source of signal/contrast: | ^13^C
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=13C+ pyruvate+ hyperpolarized)]

Pyruvate (Pyr) is an endogenous substrate enriched at a crossroad of the major energy-generating metabolic pathways in mammalian cells (1). Under most physiological conditions, the bulk of intracellular Pyr is generated endogenously by glycolysis of glucose or oxidation of lactate (Lac) (2). Pyr is then converted into several products through different metabolic pathways in mitochondria or cytoplasm (2, 3). In mitochondria, one of the major pathways is the irreversible transformation of Pyr into acetyl-coenzyme A (acetyl-CoA) and CO_2_ by pyruvate dehydrogenase (PDH) in the presence of coenzyme nicotinamide adenine dinucleotide (NAD^+^/NADH). Another major pathway is the conversion of Pyr into oxaloacetate by PDH. Both acetyl-CoA and oxaloacetate are substrates of the tricarboxylic acid cycle (TCA), also known as the Krebs cycle, which generates adenosine triphosphate (ATP) and provides energy to the cell. In the cytoplasm, Pyr is converted into alanine (Ala) by glutamine-Pyr transaminase (GPT) and reversibly oxidized back to Lac by lactate dehydrogenase (LDH). With its ability to increase cardiac mechanical performance and energy reserves, Pyr has been an important therapeutic agent in the treatment of diseases such as dysfunctional myocardium (2). Pyr is also a diagnostic marker in cancers because it is abundantly converted to Lac through anaerobic glycolysis (1). The abnormality of Pyr metabolism in diseased tissue can be detected through quantification of its metabolites. ^13^C Magnetic resonance spectroscopic imaging (MRSI) is suitable for in vivo quantification because of the inherent chemical shift dispersion of the major metabolites of Pyr (4). The chemical shift value is 178 ppm for Ala, 185 ppm for Lac, 124.5 ppm for CO_2_, and 173 ppm for Pyr itself (4). Since ^13^C has low natural abundance (1.1%) and a low gyromagnetic ratio (one quarter compared to proton spin), direct measurement of these metabolites is extremely difficult even with high magnetic fields. The recently developed hyperpolarization technique can increase the signal/noise ratio (SNR) by 10,000-fold (5), allowing direct detection of these metabolites via ^13^C MRSI.

The signal of nuclear magnetic resonance (NMR) imaging is proportional to the thermal equilibrium polarization of nuclear spins. As a function of magnetic field strength and temperature, the thermal equilibrium polarization normally is very low (i.e., 1×10^-6^ for ^13^C at 1.5 T and at body temperature). The hyperpolarization technique increases the polarization of spins by creating an artificial, non-equilibrium distribution of nuclei. Dynamic nuclear polarization (DNP) is an effective technique to hyperpolarize the ^13^C nuclei of Pyr. Electron spins have a large magnetic moment that is ~660 times stronger than the magnetic moment of proton spins. This strong magnetic moment can be transferred to proton spins through the DNP technique. Theoretically, the DNP enhancement factor for NMR signals depends on the ratio of the electronic gyromagnetic ratio to the nuclear gyromagnetic ratio (γ_e_/γ_n_) in high magnetic fields, which corresponds to a DNP enhancement factor of ~660 for ^1^H nuclei and ~2600 for ^13^C nuclei (6). There are four mechanisms accounted for in the DNP process: the Overhauser effect, the solid effect, thermal mixing, and the cross effect or electronuclear cross-polarization (7). The DNP experiments are generally conducted at low temperatures to attenuate competing spin-lattice relaxation processes and avoid loss of efficiency during the polarization transfer (9). Radicals containing unpaired electrons, which have a thermal equilibrium polarization of almost unity when exposed to a magnetic field of ~3 T at a temperature of ~1 K, are added (8). Microwave irradiation near the electron resonance frequency of the radical is used to transfer the polarization from the unpaired electrons on the radicals to the ^13^C nuclei on substrates. As a result of the short T_1_ of the electrons (~1 μs), the electrons rapidly regain their polarization. This continuous pumping process can increase the nuclear polarization in the solid material by 20–40% (8). By rapid dissolution, the solid is transformed into an injectable liquid with small polarization losses. The use of DNP produces an enhancement factor of 10^5^ in ^13^C polarization compared to the thermal equilibrium state at typical magnetic field strengths (8), allowing for direct imaging of metabolites at mM in vivo.

A major difference between the signal of hyperpolarized ^13^C and the signal of conventional NMR is that the magnetization of hyperpolarized ^13^C is created outside the magnetic field in a polarizer system (9). Once the hyperpolarization has been created, the polarization will strive to return to the thermal equilibrium level at a rate governed by T_1_ relaxation time, which typically ranges from a few seconds to several minutes for ^13^C. The corresponding time window for imaging is approximately a few minutes. Because the 1.1% natural abundance of ^13^C produces a negligible ^13^C signal, there is virtually no background signal other than noise from the patient and the coil/receiver system. The injected hyperpolarized ^13^C-labeled Pyr (HP[^13^C]Pyr) generates a ^13^C signal that is linearly proportional to its concentration. In this respect, hyperpolarized ^13^C MRI behaves in a manner similar to modalities such as positron emission tomography (PET) and single-photon emission tomography (SPECT). Neither PET nor SPECT can distinguish between metabolites and substrates. However, the large chemical shift dispersion in ^13^C MRSI can be used for quantification of each metabolite (10). The measurement of spatial distribution of metabolites via ^13^C MRSI allows the establishment of enzyme activity maps (11).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(13C+ pyruvate+ hyperpolarized)+AND+synthesis%0D%0A)]

The preparation of HP[^13^C]Pyr was described by several authors (10, 12). Two starting materials, [1-^13^C]Pyr and Tris{8-carboxyl-2,2,6,6-tetra[2-(1-hydroxyethyl)]-benzo(1,2-d:4,5-d’)bis(1,3)dithiole-4-yl}methyl sodium (trityl radical), were commercially available. Both chemicals were dissolved in an aqueous solvent and loaded into a chamber where the sample was cooled to 1.2 K at a pressure of 0.8 mbar. The sample was then irradiated with microwaves (~93.9 GHz) in a helium bath at a magnetic field of 3.35 T for >1 h. After the polarization, the sample was dissolved with hot solvents to produce an injectable solution at approximately 37°C. The level of polarization was estimated by measuring the free induction decays of an aliquot in a NMR spectrometer. The typical polarization was 20–30%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(13C+ pyruvate+ hyperpolarized)+AND+%22in+vitro%22)]

The evaluation of HP[^13^C]Pyr influx in EL-4 mouse lymphoma cells was conducted with a 9.4-T imager (11). After adding HP[^13^C]Pyr into the cells, the conversion of Pyr to Lac produced an increased Lac carboxyl signal that decayed at an apparent T_1_ of 40 s. The ^13^C peak intensities for Pyr and Lac were fitted to a modified two-site exchange Bloch equation to extract the apparent exchange rate constants. These rate constants were used to evaluate the LDH activity and Pyr influx during drug treatment. Etoposide was an inhibitor of the enzyme topoisomerase II used in chemotherapy for various malignant carcinomas. A 16-h treatment of the tumor cells with etoposide caused ~30–40% apoptosis and 10–15% necrosis in the cells. This induced ~80% reduction in Pyr flux, which was decreased from 54 ± 15 nmol/s per 10^8^ cells to 9.0 ± 1.5 nmol/s per 10^8^ cells. The LDH activity was nearly the same: 5.43 ± 0.34 units/10^7^ cells in control cells and 5.37 ± 0.27 units/10^7^ cells in drug-treated cells. A 20-h treatment with etoposide produced a 45% necrosis in the cells. The LDH activity also decreased significantly to 2.53 ± 0.32 units/10^7^ cells. The levels of necrosis and apoptosis were further confirmed by flow cytometry.

The metabolism of HP[^13^C]Pyr in isolated rat hearts was examined at 14.1 T (10). Hearts from adult rats were rapidly excised and perfused at 37°C using standard Langendorff methods. After each aorta was cannulated, each heart was placed in a NMR tube that was then filled with recirculated medium containing fatty acids and 2 mM HP[^13^C]Pyr with 20–30% polarization. Fatty acids with even or odd carbons were used to modulate the influx of PDH. Propionate (a three-carbon fatty acid) activated 90% PDH and stimulated PDH flux, whereas even-carbon fatty acid strongly inhibited PDH. Experiments were performed under ideal conditions for detected downstream metabolites such as H^13^CO_3_^-^ (160.9 ppm) and ^13^CO_2_ (124.5 ppm) in the presence of HP[^13^C]Pyr alone as well as in the presence of HP[^13^C]Pyr with even or odd fatty acids. The intensity of the H^13^CO_3_^-^ and ^13^CO_2_ resonances in the hearts reached a maximum of ~20 s after infusion of HP[^13^C]Pyr. The ratio of the H^13^CO_3_^-^ resonance area to the ^13^CO_2_ area was 7.03 ± 0.5 and remained constant until T_1_ relaxation began to destroy the ^13^CO_2_ signal. In the presence of octanoate, a medium chain fatty acid, H^13^CO_3_^-^ and ^13^CO_2_ were nearly invisible and did not recover even in the presence of propionate. This result suggested an effective competition of octanoate with Pyr for supplying acetyl-CoA to the heart.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(13C+ pyruvate+ hyperpolarized) +AND++rodentia)]

The dynamic spectra of HP[^13^C]Pyr were collected in rats at 3 T (4). Healthy rats were injected intravenously with 3 ml of HP[^13^C]Pyr solution at 79 mM in 12 s. Chemical shift imaging (CSI) of a thick slab was initiated ~30 s after the injection of HP[^13^C]Pyr with a dual-tuned volume coil was started, and the CSI were acquired every 3 s. The produced images for a 90-mm slab reflected a combined effect of metabolism, blood flow, and T_1_ relaxation. The results demonstrated that the conversion of Pyr to its metabolites, including Lac, Ala, and bicarbonate, occurred within a minute of injection. Among these metabolites, Ala was observed primarily in skeletal muscle and liver; Lac and bicarbonate were relatively concentrated in the vasculature and kidneys.

The metabolism of HP[^13^C]Pyr in lymphoma tumors was examined in mice at 9.4 T (11). After intravenous injection of 0.2 ml of HP[^13^C]Pyr solution at 75 mM within 3 s, ^13^C magnetic resonance spectroscopy (MRS) and ^13^C MRSI were used to evaluate the flux between Pyr and Lac in the tumors. A series of images was acquired to calculate an enzyme activity map. The experiments were performed in mice with and without etoposide treatment. There was a substantial signal from Pyr but only a small signal from Lac in drug-treated and untreated mice. The signal intensities were fitted to a two-site exchange Bloch equation to extract apparent exchange rate constants and spin-lattice relaxation times. A treatment with etoposide resulted in 37 ± 4% death of tumors versus 5 ± 1% in the control group. This led to ~25% reduction in the rate constant of Pyr, which decreased from 0.075 ± 0.011 s^-1^ to 0.056 ± 0.005 s^-1^. The decreased flux between Pyr and Lac were demonstrated in a plot in terms of the labeled Lac/Pyr ratio. Pyr concentration in excised tumors was 0.55 ± 0.19 μmol/g in control tumors and 0.75 ± 0.48 μmol/g in drug-treated tumors as determined by ^1^H NMR.

The metabolism of HP[^13^C]Pyr was also examined in P22 tumors implanted in six rats (1). ^13^C-Labeled CSI images were collected for a slice 10 mm thick with a 5×5-mm^2^ in-plane pixel size at 1.5 T. HP[^13^C]Pyr was infused in 14 s at a dose of 0.79 mmol/kg. The ^13^C CSI scans were acquired starting 30 s after the infusion began. All tumors showed significantly higher Lac content within 30 s than the normal tissue. The metabolic conversion of Pyr into Ala and Lac was found in all rats, but the Lac production was especially pronounced in all the tumors. HP[^13^C]Pyr was used to evaluate the Lac production in transgenic adenocarcinomas of mouse prostate (TRAMP) mice at 3 T (12). ^13^C MRI or ^13^C MRSI were collected for both primary and metastatic tumors. The primary tumors and lymph node metastases showed much higher Lac levels compared to the normal mouse prostates.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(13C+ pyruvate+ hyperpolarized) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(13C+ pyruvate+ hyperpolarized) +AND+human)]

No publication is currently available.

### NIH Support

RR 02584, HL 34557, EB005363, EB007588

## References

1 Golman K., Zandt R.I., Lerche M., Pehrson R., Ardenkjaer-Larsen J.H. (2006). Metabolic imaging by hyperpolarized 13C magnetic resonance imaging for in vivo tumor diagnosis. Cancer Res.
2 Mallet R.T. (2000). Pyruvate: metabolic protector of cardiac performance. Proc Soc Exp Biol Med.
3 Koukourakis M.I., Giatromanolaki A., Sivridis E., Gatter K.C., Harris A.L. (2005). Pyruvate dehydrogenase and pyruvate dehydrogenase kinase expression in non small cell lung cancer and tumor-associated stroma. Neoplasia.
4 Kohler S.J., Yen Y., Wolber J., Chen A.P., Albers M.J., Bok R., Zhang V., Tropp J., Nelson S., Vigneron D.B., Kurhanewicz J., Hurd R.E. (2007). In vivo 13 carbon metabolic imaging at 3T with hyperpolarized 13C-1-pyruvate. Magn Reson Med.
5 Ardenkjaer-Larsen J.H., Fridlund B., Gram A., Hansson G., Hansson L., Lerche M.H., Servin R., Thaning M., Golman K. (2003). Increase in signal-to-noise ratio of > 10,000 times in liquid-state NMR. Proc Natl Acad Sci U S A.
6 Hall D.A., Maus D.C., Gerfen G.J., Inati S.J., Becerra L.R., Dahlquist F.W., Griffin R.G. (1997). Polarization-enhanced NMR spectroscopy of biomolecules in frozen solution. Science.
7 Joo C.G., Hu K.N., Bryant J.A., Griffin R.G. (2006). In situ temperature jump high-frequency dynamic nuclear polarization experiments: enhanced sensitivity in liquid-state NMR spectroscopy. J Am Chem Soc.
8 Mansson S., Johansson E., Magnusson P., Chai C.M., Hansson G., Petersson J.S., Stahlberg F., Golman K. (2006). 13C imaging-a new diagnostic platform. Eur Radiol.
9 Olsson L.E., Chai C.M., Axelsson O., Karlsson M., Golman K., Petersson J.S. (2006). MR coronary angiography in pigs with intraarterial injections of a hyperpolarized 13C substance. Magn Reson Med.
10 Merritt M.E., Harrison C., Storey C., Jeffrey F.M., Sherry A.D., Malloy C.R. (2007). Hyperpolarized 13C allows a direct measure of flux through a single enzyme-catalyzed step by NMR. Proc Natl Acad Sci U S A.
11 Day S.E., Kettunen M.I., Gallagher F.A., Hu D.E., Lerche M., Wolber J., Golman K., Ardenkjaer-Larsen J.H., Brindle K.M. (2007). Detecting tumor response to treatment using hyperpolarized 13C magnetic resonance imaging and spectroscopy. Nat Med.
12 Chen A.P., Albers M.J., Cunningham C.H., Kohler S.J., Yen Y.F., Hurd R.E., Tropp J., Bok R., Pauly J.M., Nelson S.J., Kurhanewicz J., Vigneron D.B. (2007). Hyperpolarized C-13 spectroscopic imaging of the TRAMP mouse at 3T-initial experience. Magn Reson Med.